# ^124/131^I-Labeled apoptosis-targeting peptide-1 (ApoPep-1)

Chemical name: | ^124/131^I-Labeled apoptosis-targeting peptide-1 (ApoPep-1)
Abbreviated name: | [^124/131^I]-ApoPep-1
Synonym:
Agent Category: | Peptide
Target: | Histone H1
Target Category: | Protein
Method of detection: | Positron emission tomography (PET) with ^124^I
Source of signal / contrast: | ^124/131^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Apoptosis)]

The process of programmed cell death (apoptosis) involves the interaction of several signaling pathways in the cell, and the presence of apoptotic cells is a characteristic feature of diseases such as cancer, ischemia, and neurodegeneration (1, 2). Interestingly, the induction of apoptosis with chemotherapy or radiotherapy is essential for the treatment of cancer, and the imaging of this process can be used to monitor disease progression or the response of tumors to different therapies. Although several types of imaging agents have been evaluated to investigate apoptosis, the tracers that are most frequently used to visualize this phenomenon are radiolabeled probes based on annexin V because they have a strong affinity for phosphatidylserine (PS), which is exposed on the surface of apoptotic and necrotic cells (in normal cells PS is present mainly on the inner side of the cell membrane bilayer) (3). These probes have been reviewed by Vangestel et al. (4).

As an alternative to using annexin-based probes to detect apoptotic tissues, Wang et al. identified an apoptosis-targeting peptide-1 (ApoPep-1; amino acid (aa) sequence: CQRPPR), a hexapeptide that was shown to bind the histone H1 protein in the nucleus (the nucleus is permeable to ApoPep-1), from a phage-display peptide library (2). The peptide was labeled with ^131^I to investigate its biodistribution in normal rats, and ^124^I-labeled ApoPep-1 was evaluated with positron emission tomography (PET) for the detection of A549 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-185&Template=cellBiology) cell tumors in nude mice.

### Related Resource Links

Apoptosis-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Apoptosis+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=PET+imaging+of+Apoptosis) for PET imaging of apoptosis

Histone H1 in Online Mendelian Inheritance in Man Database (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=Human%20Histone%20H1)

Apoptosis pathways (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=Apoptosis&Submit=Go) in Pathway Interaction Database

Histone H1 in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=histone%20h1)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-ApoPep-1%20synthesis&cmd=DetailsSearch)]

The identification and isolation of the ApoPep-1 peptide from a phage peptide library has been described by Wang et al. (2). The peptide was subsequently obtained from a commercial source to perform the various investigations. The peptide was labeled with ^124/131^I using a commercially available Iodobead kit as detailed elsewhere, and the final labeled product was purified with fast protein liquid chromatography on a C-18 column (2). The radiochemical purity of ^124/131^I-ApoPep-1 was >90%, but the radiochemical yield and specific activity of the radioiodinated peptides were not reported. The purified ^124/131^I-labeled peptides were used as such (containing ~10% free iodide) for the biodistribution and microPET imaging studies. [^124/131^I]-ApoPep-1 was reported to show little degradation in serum (data not presented).

For some experiments, a fluorescein isothiocynate dye derivative of ApoPep-1 (FITC; FITC-ApoPep-1) or a Cy7.5 near-infrared dye derivative of ApoPep-1 (Cy7.5-ApoPep-1) was used (2). The FITC and Cy7.5 dyes were conjugated to the N-terminal of the peptide. The procedure used to conjugate FITC or the Cy7.5 dyes to ApoPep-1 and the purity of the dye-labeled products was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-ApoPep-1%20in%20vitro%20studies&cmd=DetailsSearch)]

The in vitro binding of ApoPep-1 to apoptotic cells was confirmed by exposing apoptosis-induced A549 and H460 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-177&Template=cellBiology) lung tumor cells and MDA-MB-231 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-26&Template=cellBiology) breast tumor cells to the FITC-conjugated peptide (2). Confocal microscopic analysis of the cells revealed that FITC-ApoPep-1 was bound only to the apoptotic cells, and this was confirmed with Alexa-488-annexin V/propidium iodide staining and flow cytometry. When the cells were pre-exposed to a mutant ApoPep-1 (R3A; aa sequence: CQAPPR), the binding of FITC-ApoPep-1 was reduced by 90%, indicating that the R3 residue in the parent peptide was most important for binding to the apoptotic cells.

Histone H1 was identified as the receptor for ApoPep-1 with the use of mass spectroscopy, fragment mapping, and colocalization assays with an anti-histone H1 antibody, as described in detail by Wang et al. (2). In addition, the anti-histone H1 antibody was shown to inhibit the binding of ApoPep-1 to apoptotic cells (cell type not mentioned) under in vitro conditions in a concentration-dependent manner.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-ApoPep-1%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^131^I]-ApoPep-1 was investigated in normal Sprague-Dawley rats (n = 4 animals/time point) (2). The rodents were injected with 0.25 MBq (7 μCi) of the radioiodinated peptide through the tail vein. The animals were euthanized at 1, 4, and 24 h post injection (p.i.), and the major organs were then collected from the rodents to measure the amount of accumulated radioactivity. Data from this study were presented as percent of injected dose per gram tissue (% ID/g). From this study, it was apparent that [^131^I]-ApoPep-1 was taken up nonspecifically by the different organs and was cleared from circulation through the kidneys within 4 h p.i. During this time, all organs, including the lungs and the liver, showed a decrease in accumulation of the label.

In vivo fluorescence imaging studies were performed on BALB/c nu/nu mice bearing A549 cell subcutaneous tumors with or without doxorubicin (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=5594d16e-72bf-4354-925e-c7591737ff1c) or camptothecin (http://www.sigmaaldrich.com/catalog/ProductDetail.do?lang=en&N4=C9911|SIGMA&N5=SEARCH_CONCAT_PNO|BRAND_KEY&F=SPEC) treatment (both of these drugs have apoptotic activity) as described by Wang et al. (2). The mice were injected with 100 nmol FITC-ApoPep-1 (for doxorubicin-treated animals) or Cy7.5-ApoPep-1 (for camptothecin-treated animals) through the tail vein, and fluorescent images were acquired from the animals at various time points. With FITC-ApoPep-1, the fluorescent signals were detected in the tumors at 1 h p.i., reached a maximum intensity at 2 h p.i., and were visible even at 4 h p.i. No signals were observed in the tumors of control animals (without doxorubicin treatment). Similar observations were reported for tumors in animals treated with Cy7.5-ApoPep-1. No blocking studies were reported.

PET images of tumors in doxorubicin-treated rats were acquired 1 h after a tail vein injection of [^124^I]-ApoPep-1 and compared to those obtained with [^18^F]-fluorodeoxyglucose ([^18^F]-FDG) (2). From the images it was clear that, compared to the control animals (no drug treatment), the uptake of [^18^F]-FDG in the tumors from the drug-treated animals increased by only 0.97-fold. However, with [^124^I]-ApoPep-1 the signal in the tumors from the doxorubicin-treated animals increased 1.6-fold compared to lesions in untreated rats. A high uptake of radioactivity was observed in the thyroid and stomach from the animals treated with [^124^I]-ApoPep-1, and the investigators attributed this to the presence of ^124^I iodide (~10% of total radioactivity, see Synthesis section above) in the injected preparation of the radioiodinated compound (2).

From these studies, the investigators concluded that radiolabeled ApoPep-1 could probably be used for the detection of apoptotic and necrotic tissues that are characteristic features of different diseases (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-ApoPep-1%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-ApoPep-1%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-ApoPep-1%20Human%20Studies)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Blankenberg F.G., Norfray J.F. (2011). Multimodality molecular imaging of apoptosis in oncology. AJR Am J Roentgenol.
2 Wang K., Purushotham S., Lee J.Y., Na M.H., Park H., Oh S.J., Park R.W., Park J.Y., Lee E., Cho B.C., Song M.N., Baek M.C., Kwak W., Yoo J., Hoffman A.S., Oh Y.K., Kim I.S., Lee B.H. (2010). In vivo imaging of tumor apoptosis using histone H1-targeting peptide. J Control Release.
3 Blankenberg F.G. (2008). In vivo detection of apoptosis. J Nucl Med.
4 Vangestel C., Peeters M., Mees G., Oltenfreiter R., Boersma H.H., Elsinga P.H., Reutelingsperger C., Van Damme N., De Spiegeleer B., Van de Wiele C. (2011). In vivo imaging of apoptosis in oncology: an update. Mol Imaging.